# L- and D-S-(3-[^18^F]fluoropropyl)homocysteine

Chemical name: | L- and D-S-(3-[^18^F]fluoropropyl)homocysteine | [image]
Abbreviated name: | L- and D-[^18^F]FPHCys | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | LAT1 amino acid transporter | [image]
Target Category: | Transporter | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of L- and D-[^18^F]FPHCys

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22SUBSTANCENAME%22%5BSubstance%5D%20AND%20Background%5BAll%20Fields%5D&cmd=DetailsSearch)]

High energy consumption and constant proliferation are the hallmarks of all cells with a malignant phenotype. To maintain a high pace of protein and DNA synthesis, such cells have an increased demand for various nutrients, glucose, and amino acids (aa). Therefore, radiotracers such as ^18^F-labeled fluorodeoxyglucose, which is taken up by the cell through the glucose transporter, are often used with positron emission tomography (PET) to detect cancerous tumors. This agent, however, is not able to distinguish between malignant tissue, inflammation, and tissues that normally have high glucose consumption, such as the brain (1). As an alternative, radiolabeled aa and their derivatives, such as those of phenylalanine and tyrosine, have been used to detect neoplastic tumors because these lesions show increased utilization of aa for the synthesis of proteins and other cellular components (2, 3). To accommodate the increased demand for aa, the malignant cells overexpress the aa transporters (phenylalanine and tyrosine use the L-type transporter), and this phenomenon promotes the rapid uptake and accumulation of the radiolabeled aa in the tumors. Therefore, noninvasive imaging with a radiolabeled aa can be used to detect cancerous lesions within a short time after administration of an aa tracer. Among the various radiolabeled aa tracers, [^18^F]-α-methyl-tyrosine is often used in the clinic, but the low yield of the final labeled product prohibits the use of this labeled compound in most oncology centers (1).

S-(2-[^11^C]methyl)-L-methionine ([^11^C]MET; half-life of ^11^C = ~20 min) is another aa derivative that is widely used for the PET imaging of tumors, but because MET contributes to a diverse array of biosynthetic reactions such as DNA synthesis, protein synthesis, etc., the radiolabeled macromolecules derived from [^11^C]MET along with the biodegradation products of the labeled molecules generate a high background signal in the tissues (4). As a consequence, the imaging of tumors with [^11^C]MET has limited utility in the clinic and this tracer has been used primarily for the noninvasive visualization of gliomas (http://www.cedars-sinai.edu/Patients/Health-Conditions/Gliomas.aspx) in the brain, and very little information is available to indicate that labeled MET is suitable for the detection of tumors in other parts of the body (3, 4). Investigators developed S-(2-[^18^F]fluoroethyl)-L-homocysteine, an analog of MET, as a possible agent for the imaging of cancerous tumors, but this agent was unstable in aqueous media and could be used for the detection of these lesions (5). In a continued effort to develop an aa derivative that can be used for the imaging of non-glioma tumors, the D and L enantiomers of S-(3-[^18^F]fluoropropyl)homocysteine ([^18^F]-D-FPHCys and [^18^F]-L-FPHCys) were synthesized, and the biodistribution and tumor imaging properties of these compounds in nude mice bearing xenograft tumors derived from different non-glioma human cancer cell lines was investigated (4, 6).

### Related Resource Links

Amino acid transporter related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporters+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Amino+acid+transporters) related to amino acid transporters

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Amino+acid+as+imaging+compound) using amino acids as imaging agents

Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D) in Online Mendelian Inheritance in Man (OMIM)

Gene information regarding L- type amino acid transporters (http://www.ncbi.nlm.nih.gov/gene/23428)

Cystinuria (http://www.cystinuria.org/resources/education/molecular_basics/) – an inherited defect of amino acid transport

Human amino acid transport disorders [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20transport%20disorders&cmd=DetailsSearch)]

Human amino acid metabolism disorders [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20amino%20acid%20metabolism%20disorders&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20synthesis&cmd=DetailsSearch)]

The synthesis of D-FPHCys and L-FPHCys and their labeling with ^18^F have been described by Bourdier et al. (4). The enantiomeric purity, radiochemical purity, and radiochemical yield of both enantiomers of [^18^F]FPHCys were typically >98%, >98%, and 20 ± 5%, respectively. The total time to prepare both tracers, from purification with high-performance liquid chromatography (HPLC), formulation, and sterile filtration through a 0.22-μm filter (for biological studies), was ~65 min. Both ^18^F-labeled compounds had a specific activity of >185 GBq/μmol (~5 Ci/μmol). The stability of the two enantiomers was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20in%20vitro&cmd=DetailsSearch)]

The uptake of [^18^F]-D-FPHCys and [^18^F]-L-FPHCys was studied in A375 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1619&Template=cellBiology) (human malignant melanoma cell line) and HT29 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (human colorectal adenocarcinoma cell line) cells (4). Radioactivity from [^18^F]-L-FPHCys was rapidly taken up by the A375 cells (with 50% of total accumulation within the initial 2 min after exposure); accumulation peaked at 60 min (9% of total dose/10^5^ cells) and gradually decreased to ~4.5% of total dose by 240 min. A similar uptake profile was observed with [^18^F]-D-FPHCys in the A375 cells; however, the initial uptake was more gradual compared to that of [^18^F]-L-FPHCys, and the maximum accumulation of label was 6.8% of total dose/10^5^ cells at 60 min after exposure, which was followed by a gradual decrease in uptake up to 240 min (~3% of total dose). The maximum uptake of [^18^F]-L-FPHCys and [^18^F]-D-FPHCys by the HT29 cells was 2% and 1.6% of total dose, respectively, at 15 min, and the accumulation decreased to ~1% of total dose for both tracers at 240 min.

From competitive inhibition experiments it was determined that the D and L labeled enantiomers of FPHCys were transported in the two cells types by the L aa transporter (LAT) system (4). In another study, [^18^F]-D-FPHCys was shown to be transported into A431 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) (human epidermoid carcinoma cell line) and Colo 205 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-222&Template=cellBiology) (human colorectal adenocarcinoma cell line) cells by the LAT1 subtype of the LAT (6). In this study, HT29 and PC3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1435&Template=cellBiology) (a human prostate adenocarcinoma cell line) cells showed a low uptake of the tracer, and both cell types were determined to have a low expression of LAT1 (as assessed with quantitative polymerase chain reaction of LAT1 mRNA). The uptake of [^18^F]-D-FPHCys by the four cell lines was shown to correlate well (R^2^ = 0.85) with the expression of LAT1 in these cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-D-FPHCys and [^18^F]-L-FPHCys was studied in nude mice bearing A375 cell xenograft tumors (n = 3 animals/group) as described by Bourdier et al. (4). Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). The amounts of tracer in the blood from [^18^F]-L-FPHCys and [^18^F]-D-FPHCys were 5.17 ± 0.18% ID/g and 3.51 ± 0.68% ID/g, 4.44 ± 0.54% ID/g and 2.51 ± 0.35% ID/g, 2.32 ± 0.33% ID/g and 0.89 ± 0.10% ID/g, and 1.38 ± 0.37% ID/g at 15, 30, 60, and 120 min postinjection (p.i.), respectively. The accumulation of radioactivity from [^18^F]-L-FPHCys in the tumor was 9.41 ± 1.21% ID/g, 8.28 ± 0.81% ID/g, 5.64 ± 0.95% ID/g, and 4.40 ± 0.67% ID/g at 15, 30, 60, and 120 min p.i., respectively. With [^18^F]-L-FPHCys, the uptake of label in the tumor was 6.01 ± 0.77% ID/g, 5.87 ± 1.14% ID/g, 3.91 ± 0.32% ID/g, and 1.68 ± 0.27% ID/g at 15, 30, 60, and 120 min p.i., respectively. The tumor/blood ratios for [^18^F]-D-FPHCys and [^18^F]-L-FPHCys at 60–120 min p.i. were ~4–5 and ~2–3, respectively. HPLC analysis showed that 90% and 80% of [^18^F]-D-FPHCys remained intact in the pancreas and urine at 60 min, respectively; however, only 30% (pancreas) and 10% (urine) of [^18^F]-L-FPHCys remained intact at the same time point. At 120 min p.i., a very low percentage (<3%) of both labeled enantiomers was incorporated into proteins of the brain, pancreas, plasma, and the tumors, indicating that the tracers had low incorporation in the macromolecules. No blocking studies were reported.

Whole-body PET images were acquired over a period of 120 min after intravenous injection of either [^18^F]-D-FPHCys or [^18^F]-L-FPHCys in nude mice bearing A375 tumors (n = 3 animals) (4). Images acquired at 60 min p.i. showed that the kidneys, followed by the tumors, had the maximum accumulation of radioactivity with both labeled compounds. Bladders of mice injected with [^18^F]-D-FPHCys showed a higher retention of radioactivity than those injected with [^18^F]-L-FPHCys. In addition, compared with [^18^F]-L-FPHCys, a lower background uptake of label from [^18^F]-D-FPHCys was observed in the liver and the muscles. No blocking studies were reported.

In another study, whole-body PET imaging was performed on nude mice bearing A431, Colo 205, PC3, or HT29 cell tumors (n = 6–10 animals/cell type) at 90 min p.i. of [^18^F]-D-FPHCys (6). From the images it was determined that the amount of radioactivity in the A431and Colo 205 cell tumors was ~3-fold higher than background, and accumulated radioactivity in the PC3 and HT29 cell tumors was ~2-fold higher than background, indicating that uptake of the label in these lesions had a high correlation (R^2^ = 0.99) with expression of the LAT1 transporter in these cells (see In Vitro Studies section for details).

From these studies, the investigators concluded that [^18^F]-D-FPHCys can be a suitable imaging agent for the detection of tumors in mice, although more work is necessary before it can be used in the clinic (4, 6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=S-%283-%5B18F%5Dfluoropropyl%29homocysteine%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kong F.L., Ali M.S., Zhang Y., Oh C.S., Yu D.F., Chanda M., Yang D.J. (2011). Synthesis and evaluation of amino acid-based radiotracer 99mTc-N4-AMT for breast cancer imaging. J Biomed Biotechnol.
2 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.
3 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: opportunities and limitations. Neuro Oncol.
4 Bourdier T., Shepherd R., Berghofer P., Jackson T., Fookes C.J., Denoyer D., Dorow D.S., Greguric I., Gregoire M.C., Hicks R.J., Katsifis A. (2011). Radiosynthesis and biological evaluation of L- and D-S-(3-[18F]fluoropropyl)homocysteine for tumor imaging using positron emission tomography. J Med Chem.
5 Bourdier T., Fookes C.J.R., Pham T.Q., Greguric I., Katsifis A. (2008). Synthesis and stability of S-(2-[18F]fluoroethyl)-L-homocysteine for potential tumour imaging. Journal of Labelled Compounds and Radiopharmaceuticals.
6 Denoyer, D., L. Kirby, K. Waldeck, P. Roselt, O.C. Neels, T. Bourdier, R. Shepherd, A. Katsifis, and R.J. Hicks, Preclinical characterization of (18)F-D-FPHCys, a new amino acid-based PET tracer. Eur J Nucl Med Mol Imaging, 2011